# Cy5.5-Amino-terminal fragment of urokinase-type plasminogen activator conjugated to magnetic iron oxide nanoparticles

Chemical name: | Cy5.5-Amino-terminal fragment of urokinase-type plasminogen activator conjugated to magnetic iron oxide nanoparticles
Abbreviated name: | Cy5.5-AFT-IO
Synonym:
Agent category: | Polypeptide
Target: | Urokinase-type plasminogen activator receptor (uPAR)
Target category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI), and optical, near-infrared (NIR) fluorescence imaging
Source of signal: | Cy5.5, iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=48146021), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=48146020) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=5329) for more information about uPAR.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ATF-IO)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used in imaging because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends primarily on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T_1_, longitudinal, and T_2_, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T1 and T_2_ relaxation times of the surrounding nuclei, mainly the protons of water. T_2_* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field [1]. Cross-linked iron oxide (CLIO) nanoparticles and other iron oxide formulations affect T_2_ primarily and lead to decreased signals. On the other hand, the paramagnetic T_1_ agents, such as gadolinium (Gd^3+^), and manganese (Mn^2+^), accelerate T_1_ relaxation and lead to brighter contrast images.

Optical fluorescence imaging is increasingly used to obtain biological functions of specific targets [2, 3] in small animals. However, the intrinsic fluorescence of biomolecules poses a problem when visible light (350-700 nm) absorbing fluorophores are used. Near-infrared (NIR) fluorescence (700-1000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in small animals.

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts [4]. Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play an important role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue [5]. Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degradation of the basement membrane and ECM [6]. Several families of proteases are involved in atherogenesis, myocardial infarction, angiogenesis, and tumor invasion and metastasis [7-10].

Urokinase-type plasminogen activator (uPA) is a serine protease [11, 12]. The uPA and uPA receptor (uPAR) system is responsible for tissue degradation after plasminogen activation to plasmin, which leads to a cascade of proteolysis or thrombolysis depending on the physiological conditions. uPA also directly activates MMPs, vascular endothelial growth factor, and human growth factor [13]. Malignant tumors and tumor-associated stromal cells (macrophages, endothelial cells and fibroblasts) often express high levels of uPA and uPAR [14]; therefore, the uPA/uPAR system is linked to vascular diseases and cancer. The amino-terminal fragment (ATF, 1-135 amino acids) of uPA binds with high affinity to uPAR [15]. Yang et al. [16] have developed a multimodality imaging probe by conjugation of Cy5.5-ATF to iron oxide nanoparticles to form Cy5.5-ATF-IO nanoparticles for NIR imaging and MRI of uPAR expression in tumor. Cy5.5 is a NIR fluorescent dye with absorbance maximum at 675 nm and emission maximum at 694 nm with a high extinction coefficient of 250,000 M^-1^cm^-1^.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=uPAR+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (uPAR (http://www.ncbi.nlm.nih.gov/gene/5329)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=uPAR)
- Clinical trials (uPAR (http://www.clinicaltrials.gov/ct2/results?term=uPAR))
- Drug information in FDA (http://google2.fda.gov/search?q=Urokinase-type+plasminogen+activator+receptor++inhibitor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=7&y=10)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ATF-IO+synthesis)]

Yang et al. [16] performed conjugation of Cy5.5 to recombinant ATF peptides with Cy5.5 maleimide. Paramagnetic iron oxide (IO) nanoparticles (10 nm core) coated with amphiphilic polymers were activated with ethyl-3-dimethylaminopropyl-carbodiimide and sulfo-N-hydroxysuccinimide for 15 min. The activated nanoparticles were incubated with Cy5.5-ATF peptides (17 kDa) at a molar iron oxide to ATF of 1:20 at 4°C overnight. Cy5.5-ATF-IO nanoparticles (18 nm in diameter) were isolated with column chromatography. There were 8-10 Cy5.5-ATF peptides per nanoparticles.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ATF-IO+and+in+vitro)]

Kim et al. [15] performed binding experiments with ATF with the use of a Biacore sensor chip immobilized with uPAR. The K_d_ value of ATF was calculated to be 122 ± 13 nM. ATF inhibited endothelial cell proliferation induced with basic fibroblast growth factor (2 ng/ml) in culture with a 50% inhibition concentration of ~320 nM. The Kd for the Cy5.5-ATF-IO was not determined. Yang et al. [16] showed that Cy5.5-ATF-IO nanoparticles exhibited T_1_-relaxivity R_1_ values of 3.6 ± 0.3 mM^-1^ s^-1^ and T_2_-relaxivity R_2_ values of 124 ± 7 mM^-1^ s^-1^ at 3 T. Cy5.5-ATF-IO nanoparticles were internalized by mouse mammary carcinoma 4T1 cells (uPAR positive) but not by human mammary carcinoma T47D cells (uPAR negative). T_2_-weighted imaging showed a signal reduction in 4T1 cells incubated with Cy5.5-ATF-IO nanoparticles compared with IO nanoparticles, whereas no signal reduction was observed in T47D cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ATF-IO+rodentia)]

Yang et al. [16] performed T_2_-weighted MR imaging (3 T) studies in mice bearing 4T1 tumors after intravenous injection of 0.2 nmol Cy5.5-ATF-IO nanoparticles. There was a 2-fold greater tumor signal reduction in the mice receiving Cy5.5-ATF-IO nanoparticles as compared with that in mice receiving IO nanoparticles at 6 h after injection. In contrast, the signal reduction was 50% and 80% less than that in mice receiving IO nanoparticles in the spleen and liver indicating non specific uptake of the IO nanoparticles. The signal reduction was similar in the kidney for both nanoparticles. Staining of iron in tissue sections confirmed the MRI findings. High resolution MR images showed the intracellular localization of nanoparticles in the cells. A high percentage of iron-positive cells were found in the tumor sections in mice injected with Cy5.5-ATF-IO nanoparticles but little or no iron-positive cells were detected in the tumor sections in mice injected with IO nanoparticles. Iron-positive cells were present in CD68-positive (macrophages) and CD68–negative cells (such as tumor cells). Optical imaging showed a strong Cy5.5 NIR fluorescence signal above the background was visualized in the tumor at 24 h after injection of Cy5.5-ATF-IO nanoparticles. The signal intensity increased at 48 h and decreased at 72 h as compared with the signal intensity at 24 h. The tumor/background ratios were 3.3, 2.2 and 2.0 at 24, 48 and 72 h, respectively. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ATF-IO+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ATF-IO+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ATF-IO+human)]

No publication is currently available.

## NIH Support

U54 CA119338, R01 CA133722, P50 CA128613

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
4 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
5 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
6 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
7 Keppler D., et al. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
8 Liu J., et al. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
9 Berchem G., et al. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
10 Brix K., et al. (2007). Cysteine cathepsins: Cellular roadmap to different functions. Biochimie.
11 Choong P.F., Nadesapillai A.P. (2003). Urokinase plasminogen activator system: a multifunctional role in tumor progression and metastasis. Clin Orthop Relat Res.
12 Rabbani S.A., Mazar A.P. (2001). The role of the plasminogen activation system in angiogenesis and metastasis. Surg Oncol Clin N Am.
13 Folkman J., Shing Y. (1992). Angiogenesis. J Biol Chem.
14 Duffy M.J., et al. (1999). Urokinase plasminogen activator: a prognostic marker in multiple types of cancer. J Surg Oncol.
15 Kim K.S., et al. (2003). Differential inhibition of endothelial cell proliferation and migration by urokinase subdomains: amino-terminal fragment and kringle domain. Exp Mol Med.
16 Yang L., et al. (2009). Receptor-targeted nanoparticles for in vivo imaging of breast cancer. Clin Cancer Res.